# Gadolinium-diethylenetriamine pentaacetic acid-GKWHCTTKFPHHYCLY

Chemical name: | Gadolinium-diethylenetriamine pentaacetic acid-GKWHCTTKFPHHYCLY
Abbreviated name: | EP-3533
Synonym:
Agent category: | Peptide
Target: | Collagen type I
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T1 relaxation and lead to increased contrast images.

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). Fibrosis is the formation of excess fibrous connective tissue (mainly collagen type I) in an organ or tissue as a reparative or reactive process in many chronic diseases in the heart, liver, kidneys, lungs, or vasculatures.

Gd, a lanthanide metal with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (4, 5). Gd-Labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and in cancer tissues. Furthermore, they are largely nonspecific. GKWHCTTKFPHHYCLY, a collagen type I binding peptide, was identified with phage display screening (6). Subsequent addition of biphenylalanine at the amidated C terminus improved collagen binding. The peptide was conjugated with three moieties of Gd-DTPA (Gd-DTPA) to form Gd-DTPA-GKWHCTTKFPHHYCLY (EP-3533) for imaging of collagen in fibrotic lesions (6, 7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+synthesis)]

GdCl_3_•6 H_2_O (2.65 mmol) was added to a solution of 2-(4-isothiocyanatobenzyl)-DTPA (ITC-DTPA, 2.65 mmol; pH 6) to form ITC-Gd-DTPA (6). GKWHCTTKFPHHYCLY (0.0133 mmol, borate buffer (pH 9)), prepared with solid-phase synthesis, was incubated with 0.18 mmol ITC-Gd-DTPA for 69 h at room temperature. The product, EP-3533, was isolated with high-performance liquid chromatography with a yield of 27%. There were three Gd molecules per EP-3533 molecule. The mass of EP-3533 was confirmed with mass spectroscopy. EP-3612 was also prepared similarly with ITC-Gd-DTPA using an inactive peptide (GKWHCTTKFPHHYCLY).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+in+vitro)]

EP-3533 exhibited r_1_ relaxivity values of 83.7 mM^-1^s^-1^ at 0.47 T and 46.8 mM^-1^s^-1^ at 1.41 T at 37°C in human plasma (6). EP-3612 showed values similar to EP-3533. The r_2_ relaxivity values were 97.5 and 101.7 mM^-1^s^-1^ at 1.41 T for EP-3533 and EP-3612, respectively. On the other hand, the relaxivity of these agents is ~15-fold higher than that of Gd-DTPA. EP-3533 exhibited a K_d_ value of 1.8 µM for collagen type I with eight binding sites per collagen molecule, whereas EP-3612 showed a K_d_ value of 400 µM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+rodentia)]

Caravan et al. (6) performed biodistribution studies in normal mice (n = 4). The organ with the highest uptake was the kidney (223 nmol Gd/g), followed by the spleen (77 nmol Gd/g), liver (50 nmol Gd/g), lung (29 nmol Gd/g), heart (26 nmol Gd/g), blood (14 nmol Gd/g), and femur (2 nmol Gd/g) at 15 min after injection of EP-3533 (10 µmol/kg). On the other hand, EP-3612 exhibited Gd levels in the blood and femur similar to EP-3533 but markedly lower levels in the other organs. MRI images (1.4 T) of collagen in a mouse model of healed myocardial infarction showed that EP-3533 enhanced T1-weighted images in the collagen-rich scar at 40 min after injection, whereas no such enhancement was observed with EP-3612. No blocking experiment was performed.

Helm et al. (7) performed dynamic T1-weighted MRI (4.7 T) studies with EP-3533 in mice (n = 8) with healed myocardial infarction. The washout time constants for EP-3533 were significantly longer than those for Gd-DTPA in regions of postinfarction scarring (194.8 ± 116.8 min versus 25.5 ± 4.2 min; P < 0.05) and in normal myocardium (45.4 ± 16.7 min versus 25.1 ± 9.7 min; P < 0.05). The washout time constants for EP-3533 and Gd-DTPA were similar in the blood (15.0 ± 2.7 min versus 17.9 ± 4.2 min, respectively). Histological staining for collagen correlated well with EP-3533–enhanced areas on MRI images. The scar tissue samples had a two-fold higher concentration of Gd than the normal myocardium at 50 min after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EP-3533+human)]

No publication is currently available.

## NIH Support

R01 EB001763, HL207284

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
5 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
6 Caravan P., Das B., Dumas S., Epstein F.H., Helm P.A., Jacques V., Koerner S., Kolodziej A., Shen L., Sun W.C., Zhang Z. (2007). Collagen-targeted MRI contrast agent for molecular imaging of fibrosis. Angew Chem Int Ed Engl.
7 Helm P.A., Caravan P., French B.A., Jacques V., Shen L., Xu Y., Beyers R.J., Roy R.J., Kramer C.M., Epstein F.H. (2008). Postinfarction myocardial scarring in mice: molecular MR imaging with use of a collagen-targeting contrast agent. Radiology.